# ^111^In-Labeled human serum albumin–conjugated Affibody Z_HER2:342_ that targets the human epidermal growth factor receptor 2 (HER2)

Chemical name: | ^111^In-Labeled human serum albumin–conjugated Affibody Z_HER2:342_ that targets the human epidermal growth factor receptor 2 (HER2)
Abbreviated name: | [^111^In]-DOTA-HSA-Z_HER2:342_
Synonym:
Agent Category: | Affibody (antibody)
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography; gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In; - vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody&cmd=DetailsSearch)]

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained by chemical synthesis or produced in bacteria with the use of recombinant technology (1). Because of their small size and high chemical and thermal stability, these molecules are used as radiolabeled probes for the targeted detection and treatment of malignant tumors as discussed elsewhere (1-3). In this regard, the epidermal growth factor receptor 2 (HER2) is considered to be an important Affibody target because it is believed to promote development of the malignant phenotype, it plays a role in the development of resistance to anticancer drugs and radiation therapy, it is overexpressed in several different cancer tumor cells, and it often indicates a poor prognosis for the patient (4). Several radionuclide-labeled Affibodies or their derivatives, such as Z_HER2:342_, have been evaluated to detect tumors expressing HER2 in preclinical studies as discussed by Tolmachev (5). Although the labeled Affibodies generate high-contrast images of the tumors, a common limitation observed with these tracers is an elevated accumulation of radioactivity in the kidneys, which masks the detection of tumors in adjacent regions of these and other organs (6). In addition, there is also a concern that the high radiation dose(s) produced from radioactivity accumulated in the kidneys can damage these organs in some patients.

Human serum albumin (HSA) is a multifunctional nonimmunogenic circulatory protein (~65 kDa) that has good biocompatible and biodegradation characteristics, and recombinant HSA (rHSA) or its derivative can be used as an excipient to formulate biological drugs (http://www.drugdeliverytech.com/ME2/dirmod.asp?nm=Back+Issues&type=Publishing&mod=Publications::Article&mid=8F3A7027421841978F18BE895F87F791&tier=4&id=E939D76B10EB4A82A10CC28C2AD08B38) (7). In addition, because HSA has a long circulating half-life and is not eliminated through the kidneys, investigators have evaluated the use of rHSA-drug conjugates to improve the efficacy of drugs and to visualize tumors using a radiolabeled integrin receptor-binding peptide coupled to rHSA (6). On the basis of this information, Hoppmann et al. evaluated the ability of a ^64^Cu- or ^111^In-labeled 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraaceticacid (DOTA)-HSA-Z_HER2:342_ Affibody conjugate to target and visualize xenograft SKOV3 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) tumors in mice with the use of positron emission tomography (PET; for the ^64^Cu-labeled Affibody) and single-photon emission tomography (SPECT; for the ^111^In-labeled Affibody), respectively. (6). This chapter describes the investigations performed with [^111^In]-DOTA-HSA-Z_HER2:342_. Studies performed with [^64^Cu]-DOTA-HSA-Z_HER2:342_ are presented in a separate chapter of MICAD (www.micad.nih.gov ) (8).

### Other Sources of Information

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Other Epidermal growth factor receptor (EGFR) imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man)

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR

Anti-EGFR antibody clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies)

EGFR pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) in Pathways Interaction Database

Production of rHSA in yeast (http://www.ncbi.nlm.nih.gov/pubmed?term=production%20of%20recombinant%20human%20serum%20albumin%20in%20yeast)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_000477.5) of human serum albumin

HSA clinical trials (http://clinicaltrials.gov/ct2/results?term=HSA)

Information regarding HSA on Food and Drug Administration web site (http://google2.fda.gov/search?q=human+serum+albumin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20synthesis&cmd=DetailsSearch)]

The synthesis of DOTA-HSA-Z_HER2:342_ and its labeling with ^111^In have been described by Hoppmann et al. (6). Approximately 2 molecules of DOTA and 1–5 molecules of Z_HER2:342_ were reported to be conjugated to each HSA molecule as determined with matrix-assisted laser desorption/ionization-time of flight-mass spectroscopy. Denaturing polyacrylamide gel electrophoresis of DOTA-HSA-Z_HER2:342_ revealed a broad band on the gel because different numbers of the Affibody molecule were attached to each molecule of HSA. The radiochemical yield of the labeled Affibody was ~60%, with a specific activity of 14–33 MBq/nmol (0.37–0.89 mCi/nmol). The [^111^In]-DOTA-HSA-Z_HER2:342_ was formulated in phosphate-buffered saline (the purification buffer, pH not mentioned), and the stability of the labeled complex was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20in%20vitro&cmd=DetailsSearch)]

The uptake of [^111^In]-DOTA-HSA-Z_HER2:342_ by SKOV3 cells was studied as described by Hoppmann et al. (6). Uptake of the radiochemical was observed to increase from 0.85 ± 0.15% (percent of added radioactivity) at 0.5 h to 1.46 ± 0.2% at 2 h. The uptake of radioactivity by the cells was significantly inhibited (P < 0.05) in the presence of excess (2.12 μM) nonradioactive Affibody. This indicated that the radiolabeled probe bound specifically to the epidermal growth factor receptor (EGFR) on the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DOTA-HSA-Z_HER2:342_ was studied in mice bearing SKOV3 cell xenograft tumors as described by Hoppmann et al. (6). The animals (n = 3 mice/group) were injected with 1.5–1.9 MBq of the tracer through the tail vein and euthanized at various time points (varying from 1 h to 48 h postinjection (p.i.)) to determine the amount of radioactivity accumulated in the major organs, including the tumors. Clearance of radioactivity from the blood was slow (~26% injected dose per gram tissue (% ID/g) and ~20% ID/g at 1 h and 4 h p.i., respectively, which decreased to 3.0 ± 0.9% ID/g at 48 h p.i.). A high uptake of the label was observed in the liver (15.6±1.8% ID/g at 4 h p.i.; this decreased to 3.6±2.9% ID/g at 48 h p.i.), but the accumulation was relatively less in the kidneys at these time points (9.9±0.7% ID/g and 5.7±0.9% ID/g at 4 h and 48 h p.i., respectively ). The accumulation of radioactivity in the tumors increased from 4.6±0.5% ID/g at 1 h p.i. to 12.5 ±1.1% ID/g at 4 h p.i. and plateaued at ~16% ID/g from 24 h to 48 h p.i. The tumor/blood ratio increased from 0.15 ± 0.06 at 1 h p.i. to 5.9 ± 2.01 at 48 h p.i., and the tumor/muscle (T/M) ratio increased from 4.09 ± 2.52 at 1 h p.i. to 16.89 ± 4.67 at 48 h p.i. This indicated that the radioactivity from the labeled Affibody was cleared from the system primarily though the hepatobiliary system. To determine the HER2 binding specificity of [^111^In]-DOTA-HSA-Z_HER2:342_, the mice were injected with the radiolabeled probe in the presence of excess nonradioactive Affibody (300 μg), and the animals were euthanized at 4 h p.i. A significantly reduced (P < 0.01) uptake of the label by the tumor was observed (6.5% ID/g in blocked versus 12.5% ID/g in the normal animals), and the T/M ratio at this time point was reduced significantly (P < 0.01) to 4.2 ± 1.6 in the blocked mice compared to a T/M ratio of 11.1 ± 1.1 in the normal group.

The tumor-targeting property of the labeled Affibody was confirmed with SPECT imaging of mice (n = 3 animals/time point) at 24 h and 48 h p.i. as detailed by Hoppmann et al. (6). Images acquired at both time points demonstrated that there was a very high accumulation of radioactivity in the tumors. The images also showed that the uptake of radioactivity by the liver was higher than that of the kidneys as observed earlier during the biodistribution studies (see above).

From this study, the investigators concluded that [^111^In]-DOTA-HSA-Z_HER2:342_ showed a high specificity for the detection of HER2-expressing tumors in rodents with the use of SPECT imaging (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-HSA-ZHER2%3A342%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Work reported in this chapter was supported in part by National Cancer Institute (NCI) grant 5R01 CA119053 and NCI In Vivo Cellular Molecular Imaging Center (ICMIC) grant P50 CA114747.

## References

1 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
2 Tolmachev V., Orlova A. (2010). Influence of labelling methods on biodistribution and imaging properties of radiolabelled peptides for visualisation of molecular therapeutic targets. Curr Med Chem.
3 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
4 Capala J., Bouchelouche K. (2010). Molecular imaging of HER2-positive breast cancer: a step toward an individualized 'image and treat' strategy. Curr Opin Oncol.
5 Tolmachev V. (2008). Imaging of HER-2 overexpression in tumors for guiding therapy. Curr Pharm Des.
6 Hoppmann S., Miao Z., Liu S., Liu H., Ren G., Bao A., Cheng Z. (2011). Radiolabeled affibody-albumin bioconjugates for HER2-positive cancer targeting. Bioconjug Chem.
7 Chuang V.T., Otagiri M. (2007). Recombinant human serum albumin. Drugs Today (Barc).
8 Chopra, A., 64Cu-Labeled human serum albumin conjugated Affibody ZHER2:342 that targets the human epidermal growth factor receptor 2 (HER2). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.